# L-[5-^11^C]-Glutamine

Chemical name: | L-[5-^11^C]-Glutamine
Abbreviated name: | L-[5-^11^C]-Gln
Synonym:
Agent category: | Compound
Target: | Neutral amino acid transporter (SLC1A5), glutaminase
Target category: | Transporter, enzyme
Method of detection: | Positron emission tomography (PET)
Source of signal: | ^11^C
Activation: | No
Studies: | - In vitro; - Rodents | Click on the above structure for additional information in PubChem (http://pubchem.ncbi.nlm.nih.gov/).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=11C%20Glutamine)]

A variety of ^11^C- and ^18^F-labeled amino acids have been studied for potential use in positron emission tomography (PET) oncology (1, 2). Most brain tumors show an increased uptake of amino acids compared with uptake in normal brain tissue (3). These amino acids are composed of naturally occurring amino acids, such as L-[^11^C]leucine, L-[^11^C]methionine (MET), and L-[^11^C]tyrosine, and of non-natural amino acids, such as [^11^C]aminoisobutyric acid, [^11^C]1-aminocyclopentane-1-carboxylic acid, and [^11^C]1-aminocyclobutane-1-carboxylic acid. ^123^I-Labeled amino acids are also used for imaging in oncology, although no radiolabeled amino acid is approved at present (1, 4, 5).

More than twenty amino acid transporter systems have been identified (1). Most of the amino acids are taken up by tumor cells through an energy-independent L-type amino acid transporter system and the Na-dependent transporter system A, as well as through the Na^+^-dependent system B^0^ (6). The amino acids are retained in tumor cells due to their high metabolic activities, including incorporation into proteins, which are higher than the metabolic activities of most normal cells (1). Malignant transformation increases the use of amino acids for energy, protein synthesis, and cell division. Tumor cells have been found to have overexpressed transporter systems (7). L-[^11^C]MET, [^18^F]fluorotyrosine, L-[^11^C]leucine, and [^18^F]fluoro-α-methyl tyrosine have been widely used in the detection of tumors (2, 6), but they are not approved by the United States Food and Drug Administration. These radiolabels are moved into cells by various amino acid transporters and are incorporated into proteins, although only leucine is quantitatively incorporated into protein. The fraction of radiolabeled amino acid that is incorporated into proteins is usually small compared to the total amount taken up into the cell. Imaging techniques that use natural amino acids are based on amino acid transport and protein incorporation.

Glutamine is utilized by proliferating cancer cells in glutaminolysis to provide energy and in synthesis of nucleotide and amino acid (8, 9). The Myc oncogene upregulates glutamine transporter (SLC1A5, neutral amino acid transporter) and glutaminase expression (10, 11). Glutaminase converts glutamine to glutamic acid, which is required for tumor growth (12). L-[5-^11^C]-Glutamine (L-[5-^11^C]-Gln) has been synthesized and evaluated as an amino acid PET tracer for the detection of tumors (13).

### Related Resource Links:

- Chapters in MICAD (Amino acid transporters (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=books&Cmd=DetailsSearch&Term=amino%20acid%20(transporter%20OR%20transporters)+AND+micad%5Bbook%5D))
- Gene information in NCBI (SLC1A5 (http://www.ncbi.nlm.nih.gov/gene/6510), glutaminase (http://www.ncbi.nlm.nih.gov/gene/2744))
- Articles in Online Mendelian Inheritance in Man (OMIM) (SLC1A5 (http://omim.org/entry/109190), glutaminase (http://omim.org/entry/138280))
- Clinical trials (Amino acid transporters (http://www.clinicaltrials.gov/ct2/results?term=amino+acid+transporters))
- Drug information in FDA (Amino acid transporters (http://google2.fda.gov/search?q=amino+acid+transporters&client=FDAgov&site=FDAgov&lr=&proxystylesheet=FDAgov&output=xml_no_dtd&getfields=*&x=13&y=15))

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=11C%20Glutamine%20and%20synthesis)]

Qu et al. (13) reported the synthesis of L-[5-^11^C]-Gln using (S)-tert-butyl 2-((tert-butoxycarbonyl)amino)-4-iodobutanoate in a two-step reaction in one pot. [^11^C]-Cyanide nucleophilic reaction was performed in the presence of KOH in dimethylformamide (120°C, 5 min), with subsequent acidic hydrolysis (120°C, 10 min) to remove the protecting groups. L-[5-^11^C]-Gln was purified with column chromatography with a radiochemical purity of >95%. The specific activity of L-[5-^11^C]-Gln was 1.85 ± 0.74 GBq/μmol (50 ± 2 mCi/μmol) at the end of synthesis, with a total synthesis time of 60 min and overall yields of 25%–40% (n = 5).

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=11C%20Glutamine%20and%20in%20vitro)]

Qu et al. (13) showed that L-[5-^11^C]-Gln entered rat glioma 9L and human glioblastoma SF188 cells cells in culture with 6% and 9% incubation dose (ID)/0.1 mg protein (n = 3) after 15 min and reached 18% and 23% ID/0.1 mg protein at 60 min, respectively. Protein incorporation at 30 min was 44.1 ± 2.3% and 26.7 ± 0.5% of the cellular uptake for 9L and SF188 cells, respectively.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=11C%20Glutamine%20and%20rodentia)]

Ex vivo biodistribution of 30 MBq (0.8 mCi) L-[5-^11^C]-Gln was studied in normal mice (n = 3/group) at 15, 30, and 60 min after injection (13). The tissue with the highest accumulation at 15 min after injection was the pancreas (7.37% injected dose/gram (ID/g)), followed by the heart (6.07% ID/g), lung (5.39% ID/g), kidney (5.34% ID/g), liver (3.99% ID/g), spleen (2.85% ID/g), blood (1.56% ID/g), brain (1.49% ID/g), and muscle (0.70% ID/g). Most tissues showed moderate to rapid washout except the pancreas. No blocking studies were performed.

Qu et al. (13) performed dynamic PET scans in rats bearing 9L tumors (66.2 MBq, 1.8 mCi) and in transgenic mice bearing spontaneous M/tomND mammary tumors (21.1 MBq, 0.6 mCi) for 60 min after injection of L-[5-^11^C]-Gln. Both tumors were clearly visualized along with the heart and abdomen area. Maximum accumulation was reached in the 9L tumors within 20 min of injection and stayed consistent for the next 40 min of imaging. On the other hand, maximum accumulation was reached in the M/tomND tumors within 5 min of imaging, and washout from the tumors was rapid for the next 55 min of imaging. No blocking studies were performed.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=11C%20Glutamine%20and%20%28dog%20or%20pig%20or%20rabbit%20or%20sheep%29)]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=11C%20Glutamine%20and%20primate%20not%20human)]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=11C%20Glutamine%20and%20human)]

No publication is currently available.

## References

1 Jager P.L., Vaalburg W., Pruim J., de Vries E.G., Langen K.J., Piers D.A. (2001). Radiolabeled amino acids: basic aspects and clinical applications in oncology. J Nucl Med.
2 Laverman P., Boerman O.C., Corstens F.H., Oyen W.J. (2002). Fluorinated amino acids for tumour imaging with positron emission tomography. Eur J Nucl Med Mol Imaging.
3 Herholz K., Heiss W.D. (2004). Positron emission tomography in clinical neurology. Mol Imaging Biol.
4 Langen K.J., Pauleit D., Coenen H.H. (2002). 3-[(123)I]Iodo-alpha-methyl-L-tyrosine: uptake mechanisms and clinical applications. Nucl Med Biol.
5 Lahoutte T., Caveliers V., Camargo S.M., Franca R., Ramadan T., Veljkovic E., Mertens J., Bossuyt A., Verrey F. (2004). SPECT and PET amino acid tracer influx via system L (h4F2hc-hLAT1) and its transstimulation. J Nucl Med.
6 Langen K.J., Jarosch M., Muhlensiepen H., Hamacher K., Broer S., Jansen P., Zilles K., Coenen H.H. (2003). Comparison of fluorotyrosines and methionine uptake in F98 rat gliomas. Nucl Med Biol.
7 Saier M.H., Daniels G.A., Boerner P., Lin J. (1988). Neutral amino acid transport systems in animal cells: potential targets of oncogene action and regulators of cellular growth. J Membr Biol.
8 Dang C.V. (2010). Glutaminolysis: supplying carbon or nitrogen or both for cancer cells?. Cell Cycle.
9 Seltzer M.J., Bennett B.D., Joshi A.D., Gao P., Thomas A.G., Ferraris D.V., Tsukamoto T., Rojas C.J., Slusher B.S., Rabinowitz J.D., Dang C.V., Riggins G.J. (2010). Inhibition of glutaminase preferentially slows growth of glioma cells with mutant IDH1. Cancer Res.
10 Dang C.V. (2010). Rethinking the Warburg effect with Myc micromanaging glutamine metabolism. Cancer Res.
11 Gao P., Tchernyshyov I., Chang T.C., Lee Y.S., Kita K., Ochi T., Zeller K.I., De Marzo A.M., Van Eyk J.E., Mendell J.T., Dang C.V. (2009). c-Myc suppression of miR-23a/b enhances mitochondrial glutaminase expression and glutamine metabolism. Nature.
12 Wang J.B., Erickson J.W., Fuji R., Ramachandran S., Gao P., Dinavahi R., Wilson K.F., Ambrosio A.L., Dias S.M., Dang C.V., Cerione R.A. (2010). Targeting mitochondrial glutaminase activity inhibits oncogenic transformation. Cancer Cell.
13 Qu W., Oya S., Lieberman B.P., Ploessl K., Wang L., Wise D.R., Divgi C.R., Chodosh L.P., Thompson C.B., Kung H.F. (2012). Preparation and Characterization of L-[5-11C]-Glutamine for Metabolic Imaging of Tumors. J Nucl Med.